# ^89^Zr-Desferrioxamine-anti-CD105 TRC105 chimeric monoclonal antibody

Chemical name: | ^89^Zr-Desferrioxamine-anti-CD105 TRC105 chimeric monoclonal antibody
Abbreviated name: | ^89^Zr-Df-TRC105
Synonym:
Agent category: | Antibody
Target: | CD105 (Endoglin, EDG)
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal/ contrast: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4557555), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=10862690) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2022) for more information about CD105

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105)]

Angiogenesis is an essential process in the development of new blood vessels both in normal physiological states and diseases (1, 2). Targeting of tumor vasculature is a promising strategy for tumor imaging and therapy because tumor growth and metastasis largely depend on angiogenesis (3-5). Transforming growth factor-β (TGF-β) is a pleiotropic cytokine that modulates blood vessel development, angiogenesis, and tumor progression (6). There are three isoforms of TGF-β (β_1_, β_2_, and β_3_). TGF-β_1_ inhibits proliferation and migration of endothelial cells and their ability to form capillaries. CD105 (endoglin, EDG) is a homodimeric transmembrane glycoprotein (180 kDa) with disulfide-linked subunits of 95 kDa. CD105 is a component of the TGF-β receptor complex that specifically binds TGF-β_1_ and TGF-β_3_ with high affinity (7). CD105 is important for blood vessel development. The expression of CD105 on different cells affects cellular response to TGF-β_1_. CD105 is overexpressed in proliferating endothelial cells of tumor vessels, and CD105 prevents TGF-β_1_-mediated inhibition of endothelial cell proliferation (8, 9).

Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (10-12). Quiescent human endothelial cells express CD105 only weakly, but the expression of CD105 is strongly upregulated on the endothelial cells of tumor tissues undergoing angiogenesis (9, 13). Anti-CD105 mAbs, such as MAEND3, E9, and MJ7/18 with radioisotopes (e.g., ^111^In, ^99m^Tc, and ^125^I) have been studied as single-photon emission computed tomography (SPECT) probes for imaging CD105 expression (9, 14). TRC105 is a human/murine chimeric IgG_1_ mAb that binds with higher affinity to human CD105 than to murine CD105 (15). TRC105 inhibits angiogenesis and tumor growth and is now in clinical trials in cancer patients. Hong et al. (16) showed that ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-anti-CD105 TRC105 (^64^Cu-DOTA-TRC105) mAbs could efficiently image 4T1 murine breast tumor in mice with positron emission tomography (PET) imaging. Hong et al. (17) also evaluated ^89^Zr-desferrioxamine-TRC105 (^89^Zr-Df-TRC105) as a ^89^Zr-based PET agent in the same 4T1 murine breast tumor model.

### Related Resource Links:

- Chapters in MICAD (CD105 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=(CD105%20OR%20endoglin)+AND+micad%5Bbook%5D))
- Gene information in NCBI (CD105 (http://www.ncbi.nlm.nih.gov/gene/2022), TGF-β_1_ (http://www.ncbi.nlm.nih.gov/gene/7040))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CD105 (http://www.ncbi.nlm.nih.gov/omim/131195), TGF-β_1_ (http://www.ncbi.nlm.nih.gov/gene/7040))
- Clinical trials (TRC105 (http://www.clinicaltrials.gov/ct2/results?term=TRC105))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+synthesis)]

Df-TRC105 was prepared by conjugation of p-isothiocyanatobenzyl-desferrioxamine B to TRC105 at a molar ratio of 3:1 (pH 9) (17). Df-TRC105 was purified with column chromatography. The number of Df moieties per mAb was not reported. Df-TRC105 was incubated with ^89^Zr-oxalate in HEPES buffer (pH 7) for 60 min at 25°C. ^89^Zr-Df-TRC105 was purified with column chromatography. This procedure provided a radiolabeling yield of 62 ± 15% (n = 10) with a specific activity of ~74 MBq/nmol (2 mCi/nmol) and a radiochemical purity of >95%. The total preparation time was ~100 min. ^89^Zr-Df-cetuximab was also prepared similarly as an isotype-matched control with similar specific activity. Cetuximab is an anti-EGFR mouse-human chimeric IgG_1_ mAb.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+in+vitro)]

Hong et al. (17) performed in vitro indirect fluorescence staining with the unlabeled TRC105 and Df-TRC105 on MCF7 human breast cancer cells (CD105-negative) and human umbilical vein endothelial cells (HUVECs, CD105-positive). Fluorescence microscopy and flow cytometry showed strong CD105 expression in HUVECs but weak or no expression in MCF7 cells. No significant differences in fluorescence intensities between TRC105 and Df-TRC105 were observed in the HUVEC cells, suggesting that Df-TRC105 retains immunoreactivity similar to that of the unconjugated mAb. ^89^Zr-Df-TRC105 was >95% intact in mouse serum after incubation for 7 days at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+in+vitro)]

Hong et al. (17) injected 5–10 MBq (0.14–0.27 mCi) ^89^Zr-Df-TRC105 into mice bearing the CD105-positive 4T1 murine breast tumors for ex vivo biodistribution and PET imaging studies (n = 4/group). Ex vivo tumor accumulation was 13% injected dose/gram (ID/g) and 6% ID/g at 24 h and 96 h after injection, respectively. The tumor/muscle ratio was 24.8 ± 4.3 at 96 h. The organ with the highest accumulation at 24 h was the liver (9% ID/g), followed by the kidney (6% ID/g), lung (4% ID/g), and spleen (3% ID/g). By 96 h, tumor accumulation was higher than that in all major organs. The radioactivity level in the blood decreased from 6.5% ID/g at 24 h to ~2.5% ID/g at 96 h. On the other hand, the accumulation of ^89^Zr-Df-cetuximab at 96 h after injection was higher or similar to that of ^89^Zr-Df-TRC105 in most organs except in the 4T1 tumors. The tumor accumulation of ^89^Zr-Df-cetuximab at 96 h after injection was 40% of ^89^Zr-Df-TRC105 tumor accumulation (P < 0.05). Injection of excess TRC105 (13 nmol) 2 h before ^89^Zr-Df-TRC105 inhibited tumor and blood radioactivity levels to the background level (<1% ID/g) at 96 h after injection. In contrast, there was a two-fold increase in liver accumulation of ^89^Zr-Df-TRC105 (P < 0.01). Immunofluorescence staining of 4T1 tumor sections showed colocalization of CD31 with CD105 on the tumor endothelial cells (CD31- and CD105-positive) but not on tumor cells (CD31-negative, CD105-positive). On the other hand, there was only weak CD105 staining on the liver and spleen sections. There was some staining in the capillaries in the medulla of the kidney sections. The accumulation of ^89^Zr-Df-TRC105 in the 4T1 tumors was largely CD105 specific, whereas accumulation in the liver and spleen was largely CD105 nonspecific.

PET imaging revealed estimated tumor accumulation of 6.1 ± 1.2% ID/g, 14.3 ± 1.2% ID/g, 12.4 ± 1.5% ID/g, 7.1 ± 0.9% ID/g, and 5.2 ± 0.3% ID/g at 5, 24, 48, 72, and 96 h after injection of ^89^Zr-Df-TRC105, respectively. Accumulation in the liver was 12.4 ± 2.1% ID/g at 5 h and declined gradually to 2.3 ± 0.1% ID/g at 96 h. The radioactivity in the blood was 14.7 ± 2.5% ID/g at 5 h and declined to 2.0 ± 0.4% ID/g at 96 h. The tumor accumulation of ^89^Zr-Df-cetuximab was <3% ID/g at 5–96 h after injection. Injection of excess TRC105 (13 nmol) 2 h before ^89^Zr-Df-TRC105 inhibited tumor accumulation to the background level (<2% ID/g) at all the time points examined. In contrast, there was a one- to two-fold increase in the radioactivity in the liver, and the radioactivity in the blood was <1% ID/g at 5–96 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TRC105+AND+human)]

No publication is currently available.

## References

1 Carmeliet P., Jain R.K. (2011). Molecular mechanisms and clinical applications of angiogenesis. Nature.
2 Folkman J. (1995). Angiogenesis in cancer, vascular, rheumatoid and other disease. Nat Med.
3 Fonsatti E., Altomonte M., Arslan P., Maio M. (2003). Endoglin (CD105): a target for anti-angiogenetic cancer therapy. Curr Drug Targets.
4 Abdollahi A., Folkman J. (2010). Evading tumor evasion: current concepts and perspectives of anti-angiogenic cancer therapy. Drug Resist Updat.
5 Thorpe P.E. (2004). Vascular targeting agents as cancer therapeutics. Clin Cancer Res.
6 Massague J., Cheifetz S., Laiho M., Ralph D.A., Weis F.M., Zentella A. (1992). Transforming growth factor-beta. Cancer Surv.
7 Cheifetz S., Bellon T., Cales C., Vera S., Bernabeu C., Massague J., Letarte M. (1992). Endoglin is a component of the transforming growth factor-beta receptor system in human endothelial cells. J Biol Chem.
8 Tabata M., Kondo M., Haruta Y., Seon B.K. (1999). Antiangiogenic radioimmunotherapy of human solid tumors in SCID mice using (125)I-labeled anti-endoglin monoclonal antibodies. Int J Cancer.
9 Bredow S., Lewin M., Hofmann B., Marecos E., Weissleder R. (2000). Imaging of tumour neovasculature by targeting the TGF-beta binding receptor endoglin. Eur J Cancer.
10 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
11 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
12 Kowalsky, R.J., S.W. Falen, Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. 2004, Washington, D.C.: APhA. 733-752.
13 Seon B.K., Haba A., Matsuno F., Takahashi N., Tsujie M., She X., Harada N., Uneda S., Tsujie T., Toi H., Tsai H., Haruta Y. (2011). Endoglin-targeted cancer therapy. Curr Drug Deliv.
14 Fonsatti E., Jekunen A.P., Kairemo K.J., Coral S., Snellman M., Nicotra M.R., Natali P.G., Altomonte M., Maio M. (2000). Endoglin is a suitable target for efficient imaging of solid tumors: in vivo evidence in a canine mammary carcinoma model. Clin Cancer Res.
15 Tsujie M., Tsujie T., Toi H., Uneda S., Shiozaki K., Tsai H., Seon B.K. (2008). Anti-tumor activity of an anti-endoglin monoclonal antibody is enhanced in immunocompetent mice. Int J Cancer.
16 Hong H., Yang Y., Zhang Y., Engle J.W., Barnhart T.E., Nickles R.J., Leigh B.R., Cai W. (2011). Positron emission tomography imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
17 Hong, H., G.W. Severin, Y. Yang, J.W. Engle, Y. Zhang, T.E. Barnhart, G. Liu, B.R. Leigh, R.J. Nickles, and W. Cai, Positron emission tomography imaging of CD105 expression with (89)Zr-Df-TRC105. Eur J Nucl Med Mol Imaging, 2011